# ^11^C-Labeled 1,7β,10β-trihydroxy-9-oxo-5β,20-epoxytax-11-ene-2α,4,13α-triyl 4-acetate 2-benzoate 13-{(2R,3S)-3-[(tert-butoxycarbonyl)amino]-2-hydroxy-3-phenylpropanoate}

Chemical name: | ^11^C-Labeled 1,7β,10β-trihydroxy-9-oxo-5β,20-epoxytax-11-ene-2α,4,13α-triyl 4-acetate 2-benzoate 13-{(2R,3S)-3-[(tert-butoxycarbonyl)amino]-2-hydroxy-3-phenylpropanoate}
Abbreviated name: | [^11^C]-Docetaxel
Synonym:
Agent Category: | Compound
Target: | Tubulin (microtubules)
Target Category: | Other (cytoskeleton)
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on above structure of docetaxel for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11c%5Ddocetaxel&cmd=DetailsSearch)]

Docetaxel (http://www.taxotere.com/oncology/about_Taxotere/default.aspx) is a diterpine (taxane) anti-mitotic agent that binds to free tubulin and leads to the assembly of stabilized microtubule bundles, inhibition of the cell cycle, and cell death due to apoptosis (1). This drug has been approved by the United States Food and Drug Administration as a single-agent treatment of metastatic breast cancer, metastatic androgen-independent prostate cancer, and advanced non-small cell lung cancer (NSCLC), and as an adjuvant in combination with doxorubicin and cyclophosphamide for the treatment of early-stage breast cancer (2). Patients treated with docetaxel often experience drug-related toxicity (due to myelosuppression) and show limited or no response to the treatment (3). To some extent, the response to an anti-neoplastic drug, including docetaxel, depends on attaining a sufficiently high concentration in the cancerous lesions, so it is important to quantify the uptake of an anti-cancer agent by the affected tissues to assess the efficacy of a drug. Therefore, measuring the amount of radionuclide-labeled docetaxel that has accumulated in cancerous tumors can be of prognostic value to predict patient response to the treatment (4). For this, ^11^C-labeled docetaxel ([^11^C]-docetaxel) was synthesized (5), and in a preliminary study its biodistribution was investigated in normal rats (4). In another study, the biodistribution and radio-dosimetry of [^11^C]-docetaxel was investigated in cancer patients (6), and recently the kinetics of [^11^C]-docetaxel was studied using positron emission tomography (PET) in lung cancer patients (3).

### Related Resource Links

Microtubule inhibitors in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=microtubule%20inhibitors&cmd=DetailsSearch)

Anti-mitotic agents in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-mitotic%20agents&cmd=DetailsSearch)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=docetaxel) with docetaxel

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5Ddocetaxel%20synthesis&cmd=DetailsSearch)]

The radiosynthesis of [^11^C]-docetaxel has been described by van Tilburg et al. (5). The decay-corrected radiochemical yield (RCY) of the reaction was 10 ± 1% (n = 5 reactions). The radiochemical purity (RCP), specific activity, and stability of the final product were not reported.

[^11^C]-Docetaxel was also synthesized as described by van Tilburg et al. with a semi-automated method compliant with good manufacturing practices (7). The total synthesis time was 67 min, with a decay-corrected RCY of 10 ± 2%, an RCP of >98%, and a SA of 9–17 GBq/ μmol (0.24–0.46 Ci/μmol) (n = 7 reactions).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=docetaxel%20in%20vitro%20cytotoxicity&cmd=DetailsSearch)]

The concentration of non-radiolabeled docetaxel that inhibits the proliferation of human SKOV-3 ovarian tumor cells by 50% (IC_50_) after 72 h drug exposure was reported by Lu et al. to be 3.4 × 10−^3^ μM (8).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=docetaxel%20rodentia&cmd=DetailsSearch)]

In a letter to the editor (no data presented), van der Velt et al. reported preliminary results obtained from a study to investigate the biodistribution of [^11^C]-docetaxel in normal rats (4, 5). The investigators reported that >99% of the injected [^11^C]-docetaxel was cleared from blood circulation in <5 min. The spleen showed the highest uptake of the labeled drug, followed by the urine, lung, and liver. Lowest uptake was observed in the brain and the testis of the animals.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=docetaxel%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=docetaxel%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11%5Ddocetaxel%20humans&cmd=DetailsSearch)]

The biodistribution and radiation dosimetry of [^11^C]-docetaxel was studied in seven cancer patients with advanced solid tumors (five individuals had NSCLC, one had malignant pleural mesothelioma, and one had prostate cancer) as described by van der Veldt et al. (6). The patients were given dexamethasone before the administration of a single intravenous bolus of 178 ± 79 MBq (4.8 ± 2.1 mCi) [^11^C]-docetaxel. Four whole-body serial PET scans were then acquired from each patient within 1 h, and the duration of each scan was 6.9 ± 1.2, 12.6 ± 2.3, 18.3 ± 3.3, and 24.0 ± 2.3 min, respectively. Regions of interest (ROI) were drawn on the PET scans for each organ, including the tumors, and the mean standardized uptake value (SUV) normalized to the body weight and the percent of the injected dose (% ID) for each organ were calculated as described elsewhere (6). High uptake of [^11^C]-docetaxel was observed in the liver (47 ± 9% ID) and the gall bladder (7.2 ± 3.6% ID), and the highest accumulated amount was observed in the gall bladder (SUV_mean_ 96 ± 49), followed by the liver (SUV_mean_ 24 ± 3) and upper large intestines (SUV_mean_ 9 ± 6). The lowest activity was detected in the brain (SUV_mean_ 0.05 ± 0.03) and the lungs (SUV_mean_ 0.7 ± 0.2). The clearance of [^11^C]-docetaxel from circulation was very rapid, and the amount of label in the blood was reported to decrease to <0.001% ID/ml within 30 min after injection.

Time-activity curves were generated from the ROI on the PET scan of one tumor from each patient, and the SUV for the tumor was calculated as detailed elsewhere (6). The highest SUV was 5.1 for a primary NSCLC tumor, and the lowest SUV was ~1.2 for a metastasized NSCLC tumor.

The liver and gall bladder had the highest estimated absorbed radiation doses of 35.2 ± 6.6 and 34.6 ± 9.9 μGy/MBq (μGy/27 μCi), respectively (6). The mean effective dose of [^11^C]-docetaxel was estimated to be 4.7 ± 0.2 μSv/MBq (μSv/27 μCi).

From this study, the investigators concluded that, because the lungs showed a low uptake of [^11^C]-docetaxel, this tracer could be used to detect tumors in the thoracic region of cancer patients (6).

In another study, the quantification of [^11^C]-docetaxel with dynamic PET-computed tomography (CT) was assessed in 34 lung cancer patients (3). The effects of tumor size, tumor perfusion, and pre-administration of dexamethasone in the patients on [^11^C]-docetaxel kinetics were also investigated in this study. Results from this study showed that the quantification of [^11^C]-docetaxel with non-invasive imaging techniques such as PET/CT is possible. The investigators were able to identify 32 lesions in the various patients, and the net variable influx rate of [^11^C]-docetaxel in these lesions was in the range of 0.0023–0.0229 mL/cm−^3^ per min−^1^. From this study, the investigators concluded that perfusion (Spearman’s p = 0.815, P < 0.001) and not size (Spearman’s p = −0.14, P < 0.446) affected the tumor uptake of [^11^C]-docetaxel. It was observed that tumors in patients pretreated with dexamethasone (n = 24 individuals) showed a lower accumulation of the tracer (P = 0.013). In addition, in a sub-group of patients treated with docetaxel, a high tumor uptake of [^11^C]-docetaxel correlated with an improved response to the drug.

From these studies, the investigators concluded that [^11^C]-docetaxel kinetics can be studied with non-invasive imaging techniques in a clinical setting, and that such investigations can reveal the sensitivity of lung cancer to therapy with this drug (3).

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Lyseng-Williamson K.A., Fenton C. (2005). Docetaxel: a review of its use in metastatic breast cancer. Drugs.
2 Sanofi-Aventis, U., Taxotere® Prescribing Information. 2010
3 van der Veldt A.A., Lubberink M., Greuter H.N., Comans E.F., Herder G.J., Yaqub M., Schuit R.C., van Lingen A., Rizvi S.N., Mooijer M.P., Rijnders A.Y., Windhorst A.D., Smit E.F., Hendrikse N.H., Lammertsma A.A. (2011). Absolute Quantification of [11C]docetaxel Kinetics in Lung Cancer Patients Using Positron Emission Tomography. Clin Cancer Res.
4 van der Veldt A.A., Lammertsma A.A., Hendrikse N.H. (2007). [11C]docetaxel and positron emission tomography for noninvasive measurements of docetaxel kinetics. Clin Cancer Res.
5 van Tilburg E.W., Franssen E.J.F., van der Hoeven J.J.M., van der Meij M., Elshove D., Lammertsma A.A., Windhorst A.D. (2004). Radiosynthesis of [11C]docetaxel. Journal of Labelled Compounds and Radiopharmaceuticals.
6 van der Veldt A.A., Hendrikse N.H., Smit E.F., Mooijer M.P., Rijnders A.Y., Gerritsen W.R., van der Hoeven J.J., Windhorst A.D., Lammertsma A.A., Lubberink M. (2010). Biodistribution and radiation dosimetry of 11C-labelled docetaxel in cancer patients. Eur J Nucl Med Mol Imaging.
7 van Tilburg E.W., Mooijer M.P., Brinkhorst J., van der Meij M., Windhorst A.D. (2008). Improved and semi-automated GMP-compliant radiosynthesis of [11C]docetaxel. Appl Radiat Isot.
8 Lu H.F., Sun X., Xu L., Lou L.G., Lin G.Q. (2009). Design, synthesis and biological evaluation of novel fluorinated docetaxel analogues. Eur J Med Chem.